# DY-675-g7-Poly(lactic-co-glycolic acid) nanoparticles

Chemical name: | DY-675-g7-Poly(lactic-co-glycolic acid) nanoparticles
Abbreviated name: | DY-g7-PLGA NPs, DY-g7-PLGA
Synonym:
Agent category: | Peptide
Target: | Opioid receptors
Target category: | Receptor
Method of detection: | Optical, near-infrared fluorescence (NIR) imaging
Source of signal: | DY-675
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=g7%20PLGA)]

Optical fluorescence imaging is increasingly being used to monitor biological functions of specific targets (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (~700–1,000 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, attributable to low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a non-invasive complement to radionuclide imaging in small animals.

Opioids such as morphine are analgesics that are commonly used in clinical practice. Three opioid receptors (mu, µ; delta, δ; and kappa, κ) that mediate opioid effects have been identified by molecular cloning: δ (enkephalin-preferring), κ (dynorphin-preferring), and µ (morphine- and ß-endorphin–preferring) (4). Each type of opioid receptor consists of subtypes of receptors as suggested by pharmacological studies (5, 6). These receptors exhibit apparent specificity to both the central and peripheral nervous systems, and their presence is ubiquitous in these systems. The opioid receptors (G-protein–coupled, resulting in decreased adenylyl cyclase activity) play an important role in the regulation of analgesia, shock, appetite, thermoregulation, and cardiovascular, mental, and endocrine function (5-8). Although µ opioid receptors are the major receptors to mediate the analgesic effects of opioids, δ and κ receptors are also important in antinociception. Opioids have been found to protect cells from ischemic injury in the heart and brain via the δ receptors. On the other hand, κ antagonists prevent neurodegeneration.

The µ opioid receptors are localized predominately in the hypothalamus and thalamus, and the δ opioid receptors are localized predominately in the striatum, limbic system, and cerebral cortex (9, 10). The κ opioid receptors (κ1 and κ2) are the most abundant brain opioid receptors and are widely distributed in deeper layers of the neocortex (particularly temporal, parietal, and frontal cortices), striatum, amygdala, and thalamus, with lower levels in the hippocampus, occipital cortex, and cerebellum (11-13). The κ opioid receptors have been implicated in several clinical brain disorders, including drug abuse (14), epilepsy (15), Tourette’s syndrome (16), and Alzheimer’s disease (17). Tyr-D-Thr-Gly-Phe-Leu-Ser-(O-β-D-Glucose)CONH2 (g7) is a glycosylated derivative of the Leu-enkephalin analog Tyr-D-Thr-Gly-Phe-Leu-Ser-CONH2 (18). The g7 peptide exhibits an agonistic activity to rat and human µ/δ opioid receptors and an ability to penetrate the blood–brain barrier (BBB). Tosi et al. (19) conjugated g7 and the NIR dye DY-675 to poly(lactic-co-glycolic acid) (PLGA) nanoparticles (NPs) to form DY-g7-PLGA NPs for in vivo NIR imaging of the BBB.

### Related Resource Links:

- Chapters in MICAD (opioid receptors (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=opioid+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad))
- Gene information in NCBI (µ opioid receptor (http://www.ncbi.nlm.nih.gov/gene/4988), δ opioid receptor (http://www.ncbi.nlm.nih.gov/gene/4985))
- Articles in Online Mendelian Inheritance in Man (OMIM) (µ opioid receptor (http://www.ncbi.nlm.nih.gov/omim/600018), δ opioid receptor (http://www.ncbi.nlm.nih.gov/omim/165195))
- Clinical trials (opioid receptors (http://www.clinicaltrials.gov/ct2/results?term=opioid+receptors+))
- Drug information in FDA (opioid receptors (http://google2.fda.gov/search?q=opioid+receptor&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=14&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=g7%20PLGA%20and%20synthesis)]

DY-g7-PLGA NPs were prepared by mixing a solution of g7-PLGA, DY-PLGA, and PLGA (1:1.5:1.5, w:w:w) in acetone with 25 ml water containing Pluronic F68 (100 mg) (19). DY-g7-PLGA NPs were isolated with column chromatography. Laser particle-size analysis showed that the mean diameter of the NPs in water solution was ~200 nm. The surface charge was negative in all NPs. DY-g7-PLGA NPs exhibited an excitation maximum at 633 nm and an emission maximum at 700 nm. The chemical purity and final ratios of components specifically the number of DY fluorescent molecules and g7 opioids per NP were not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=g7%20PLGA%20and%20in%20vitro)]

Elmagbari et al. (18) reported that g7 exhibited 50% inhibition concentrations of 8.16 nM and 3.35 nM for µ and δ opioid receptors, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=g7%20PLGA%20and%20rodentia)]

Tosi et al. (19) used a whole-body fluorescence detection system to perform in vivo time-domain optical imaging at 0, 0.1, 1, and 2 h after intravenous injection of DY-g7-PLGA NPs (8 mg/mouse) in normal mice. Fluorescence signal was first observed in the blood circulation with subsequent localization to the brain, lungs, and liver within a few minutes after injection. The fluorescence intensity in the brain stayed constant over time, whereas the fluorescence intensity in the lung and liver migrated to the abdominal region within 1 h. The fluorescence intensity in the brain was weaker than that in the lungs and liver. Fluorescent and confocal microscopy studies of the brain sections showed that DY-g7-PLGA NPs localized very close to nuclear structures of the brain cells at 3 h after injection, suggesting that DY-g7-PLGA NPs were able to cross the BBB. DY-PLGA NPs were not tested as a control. No blocking studies to demonstrate specificity were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=g7%20PLGA%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=g7%20PLGA%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=g7%20PLGA%20and%20human)]

No publication is currently available.

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Minami M., Satoh M. (1995). Molecular biology of the opioid receptors: structures, functions and distributions. Neurosci Res.
5 Waldhoer M., Bartlett S.E., Whistler J.L. (2004). Opioid receptors. Annu Rev Biochem.
6 Satoh M., Minami M. (1995). Molecular pharmacology of the opioid receptors. Pharmacol Ther.
7 Molina P.E. (2006). Opioids and opiates: analgesia with cardiovascular, haemodynamic and immune implications in critical illness. J Intern Med.
8 Barry U., Zuo Z. (2005). Opioids: old drugs for potential new applications. Curr Pharm Des.
9 Chang K.J., Cooper B.R., Hazum E., Cuatrecasas P. (1979). Multiple opiate receptors: different regional distribution in the brain and differential binding of opiates and opioid peptides. Mol Pharmacol.
10 Pfeiffer A., Pasi A., Mehraein P., Herz A. (1982). Opiate receptor binding sites in human brain. Brain Res.
11 Peckys D., Landwehrmeyer G.B. (1999). Expression of mu, kappa, and delta opioid receptor messenger RNA in the human CNS: a 33P in situ hybridization study. Neuroscience.
12 Hiller J.M., Fan L.Q. (1996). Laminar distribution of the multiple opioid receptors in the human cerebral cortex. Neurochem Res.
13 Simonin F., Gaveriaux-Ruff C., Befort K., Matthes H., Lannes B., Micheletti G., Mattei M.G., Charron G., Bloch B., Kieffer B. (1995). kappa-Opioid receptor in humans: cDNA and genomic cloning, chromosomal assignment, functional expression, pharmacology, and expression pattern in the central nervous system. Proc Natl Acad Sci U S A.
14 Mello N.K., Negus S.S. (2000). Interactions between kappa opioid agonists and cocaine. Preclinical studies. Ann N Y Acad Sci.
15 de Lanerolle N.C., Williamson A., Meredith C., Kim J.H., Tabuteau H., Spencer D.D., Brines M.L. (1997). Dynorphin and the kappa 1 ligand [3H]U69,593 binding in the human epileptogenic hippocampus. Epilepsy Res.
16 Chappell P.B., Leckman J.F., Scahill L.D., Hardin M.T., Anderson G., Cohen D.J. (1993). Neuroendocrine and behavioral effects of the selective kappa agonist spiradoline in Tourette's syndrome: a pilot study. Psychiatry Res.
17 Mathieu-Kia A.M., Fan L.Q., Kreek M.J., Simon E.J., Hiller J.M. (2001). Mu-, delta- and kappa-opioid receptor populations are differentially altered in distinct areas of postmortem brains of Alzheimer's disease patients. Brain Res.
18 Elmagbari N.O., Egleton R.D., Palian M.M., Lowery J.J., Schmid W.R., Davis P., Navratilova E., Dhanasekaran M., Keyari C.M., Yamamura H.I., Porreca F., Hruby V.J., Polt R., Bilsky E.J. (2004). Antinociceptive structure-activity studies with enkephalin-based opioid glycopeptides. J Pharmacol Exp Ther.
19 Tosi G., Bondioli L., Ruozi B., Badiali L., Severini G.M., Biffi S., De Vita A., Bortot B., Dolcetta D., Forni F., Vandelli M.A. (2011). NIR-labeled nanoparticles engineered for brain targeting: in vivo optical imaging application and fluorescent microscopy evidences. J Neural Transm.